# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-HHEAYGWMDF-NH_2_ peptide

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-HHEAYGWMDF-NH_2_ peptide
Abbreviated name: | ^111^In-DOTA-H2-Met
Synonym: | Radiolabeled minigastrin
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2, CCK-B) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal/contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about.the CCK-2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29)]

^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-HHEAYGWMDF-NH_2_ peptide (^111^In-DOTA-H2-Met) is a radiolabeled gastrin analog that can be used for single-photon emission computed tomography (SPECT) imaging of tumors that express the gastrin/cholecystokinin-2 (CCK-2) receptor (1). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The gastrointestinal peptides gastrin and CCK have various regulatory functions in the brain and gastrointestinal tract (2). Gastrin and CCK have the same COOH-terminal pentapeptide amide sequence, which is the biologically active site (3). Human gastrin is a peptide composed of 34 amino acids and also exists in several C-terminal truncated forms (1). These C-terminal truncated forms include minigastrin, which is a 13-residue peptide with the sequence of LEEEEEAYGWMDF-NH_2_. CCKs exist in a variety of biologically active molecular forms that are derived from a precursor molecule comprising 115 amino acids (4). These forms range from 4 to 58 amino acids in length and include sulphated and unsulphated CCK-8, which has the structure DYMGWMDF-NH_2_. They bind to and act through transmembrane G-protein–coupled receptors (5). Two different CCK receptor subtypes have been identified in normal tissues. CCK-1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK-2 (CCK-B, brain) receptors have high affinity for gastrin (4). They also differ in terms of molecular structure, distribution, and affinity for CCK. These receptors have also been found to be expressed or overexpressed on a multitude of tumor types (5). CCK-2 receptors have been found most frequently in medullary thyroid carcinoma, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (2). CCK-1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastoma.

Reubi et al. (6) designed a series of radiolabeled CCK-8 peptides that showed high specificity for potential in vivo imaging of tumors expressing CCK-2 receptors. de Jong et al. (7) developed an ^111^In-labeled non-sulfated CCK8 analog that used 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) as a bifunctional chelating agent. The radioligand showed high specific internalization rates in receptor-positive AR42J rat pancreatic tumor cells. von Guggenberg et al. (8) reported the synthesis of ^99m^Tc-hydrazinonicotinic acid (HYNIC)-minigastrin complexes and showed high tumor uptake in nude mice bearing AR42J tumors. Nock et al. (9) prepared ^99m^Tc-labeled minigastrin analogs and found that they displayed high specific localization in nude mice bearing AR42J tumors. Mather et al. (1) synthesized a library of different peptide sequences based on the C-terminal sequences of CCK-8 or minigastrin. These peptides were labeled with ^111^In by DOTA or diethylenetriamine pentaacetic acid (DTPA) conjugation. Although their ultimate goal was to identify an analog that could be used for radiotherapeutic applications, ^111^In-DOTA-H2-Met appeared to have the best pharmacokinetic properties with the highest tumor/kidney ratio and low uptake by nontarget tissues.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20synthesis)]

The peptide sequence HHEAYGWMDF-amide was obtained by solid-phase peptide synthesis under standard conditions from commercial sources (1). The N-terminus was capped with a DOTA chelating group to produce DOTA-H2-Met. The identity and purity were confirmed by matrix-assisted laser desorption/ionization mass spectroscopy and reverse-phase high-performance liquid chromatography (HPLC). Radiolabeling was performed by mixing ^111^In-chloride in ammonium acetate and 0.04-M monothioglycerol (MTG), an antioxidant, with DOTA-H2-Met in 0.01-M phosphate-buffered saline (pH 7.2). The mixture was heated at 98ºC for 15 min, and 0.1-M ethylenediamine tetraacetic acid (EDTA) was then added to quench the reaction. The labeling efficiency was >90%. The radiochemical purity was not reported, but HPLC chromatography of MTG-added samples showed a single peak with a small peak of 5.9% identified as the oxidized peptide. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20in%20vitro)]

In the in vitro plasma stability study, ^111^In-DOTA-H2-Met was incubated with fresh human blood at 37ºC (1). HPLC analysis showed that >95% of intact peptide remained after 4 h incubation, but only 62% remained after 24 h. In comparison, 98% of the radioligand remained intact in phosphate-buffered saline after 24 h. An in vitro receptor affinity assay was performed by using AGS human gastric tumor cells transfected with the CCK-2 receptor (AGS-CCK2R) and ^125^I-G17 as the radioligand. The inhibition constant (K_i_) and half of the maximum binding fraction (EC_50_) were 3.9 nM and 5.7 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20rodentia)]

Biodistribution studies of ^111^In-DOTA-H2-Met were performed in nude mice bearing AR42J rat pancreatic tumors (1), HT29 human colorectal tumors, or CA20948 rat pancreatic tumors. Both AR42J and CA20948 tumors expressed different levels of gastrin receptors, and HT29 was a cell line transfected with a relatively low level of gastrin receptors. Each mouse received 0.2 μg of ^111^In-DOTA-H2-Met by i.v. injection. The tumor radioactivity levels at 4 h (n = 3–4), represented as percent injected dose per g (% ID/g), were 0.87 ± 0.21, 0.59 ± 0.10, and 0.19 ± 0.05 for AR42J, CA20948, and HT29 tumors, respectively. The radioactivity in the AR42J tumor reached ~2% ID/g at 1 h (Figure 1), and then decreased to ~0.5% ID/g in 72 h. With the coadministration of 100 μg of unlabeled peptide, the radioactivity level in the AR42J tumor at 4 h was reduced to ~0.1−0.2% ID/g. The blood clearance was extremely rapid, and there was a gradual washout from all tissues. The blood radioactivity levels at 4 h were 0.04 ± 0.01, 0.07 ± 0.02, and 0.08 ± 0.01 for AR42J, CA20948, and HT29 tumors, respectively. The kidney levels at 4 h were 1.87 ± 0.60, 2.41 ± 0.91, and 2.44 ± 0.47 for AR42J, CA20948, and HT29 tumors, respectively. The tumor/kidney ratios were 0.47 (n = 15), 0.24 (n = 7), and 0.08 (n = 6) for AR42J, CA20948, and HT29 tumors, respectively. A dose-ranging study showed that the peptide dose >1 μg appeared to reduce the tumor uptake.

Gamma imaging of ^111^In-DOTA-H2-Met in mice bearing AR42J tumors showed an uptake pattern that was similar to that of the biodistribution studies (1). There was a modest level of tumor uptake with heterogeneous distribution within the tumor mass. There was little uptake in the central organs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20human)]

No publication is currently available.

## References

1 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
2 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
3 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 Reubi J.C., Waser B. (1996). Unexpected high incidence of cholecystokinin-B/gastrin receptors in human medullary thyroid carcinomas. Int J Cancer.
7 de Jong M., Bakker W.H., Bernard B.F., Valkema R., Kwekkeboom D.J., Reubi J.C., Srinivasan A., Schmidt M., Krenning E.P. (1999). Preclinical and initial clinical evaluation of 111In-labeled nonsulfated CCK8 analog: a peptide for CCK-B receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
8 von Guggenberg E., Behe M., Behr T.M., Saurer M., Seppi T., Decristoforo C. (2004). 99mTc-labeling and in vitro and in vivo evaluation of HYNIC- and (Nalpha-His)acetic acid-modified [D-Glu1]-minigastrin. Bioconjug Chem.
9 Nock B.A., Maina T., Behe M., Nikolopoulou A., Gotthardt M., Schmitt J.S., Behr T.M., Macke H.R. (2005). CCK-2/gastrin receptor-targeted tumor imaging with (99m)Tc-labeled minigastrin analogs. J Nucl Med.